# ^18^F-Labeled neogalactosylalbumin

Chemical name: | ^18^F-Labeled neogalactosylalbumin | [image]
Abbreviated name: | [^18^F]FNGA | [image]
Synonym: | | [image]
Agent Category: | Protein | [image]
Target: | Asialoglycoprotein receptor (ASGP-R) | [image]
Target Category: | Receptor | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of [^18^F]FNGA according to Yang et. al. (1). Click here for human asialoglycoprotein receptor 1 nucleotide and protein sequence (http://www.ncbi.nlm.nih.gov/nuccore/AB070933.1?ordinalpos=9&itool=EntrezSystem2.PEntrez.Sequence.Sequence_ResultsPanel.Sequence_RVDocSum).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Asialoglycoprotein+receptors)]

Asialoglycoprotein receptors (ASGP-R; exist as subtypes 1 and 2) are located on the surface of hepatic cell membranes and are involved in the binding and endocytosis of glycoproteins that have exposed carbohydrate or N-acetylgalactosamine residues (2). In addition, the decreased level of ASGP-R on the hepatic cells has been shown to correlate clinically with the degree of liver function retained due to the development of cirrhosis, cancer, or viral hepatitis (2). Therefore, ^99m^Tc-labeled galactosyl human serum albumin (HSA), a single-photon emission computed tomography (SPECT) imaging agent that targets the ASGP-R, was developed and evaluated, and it is commercially available in Japan for clinical diagnosis of diseases of the liver or to assess the hepatic functional status (1). As an alternative to the SPECT imaging compound, Yang et al. developed ^18^F-labeled neoglycoalbumin ([^18^F]FNGA) for imaging of the liver with positron emission tomography (PET) (1). The biodistribution of [^18^F]FNGA was studied in normal mice with or without pretreatment of non-radioactive NGA. In addition, imaging was performed on rats treated with [^18^F]FNGA in the presence or absence of non-labeled NGA.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FNGA+synthesis)]

The synthesis of [^18^F]FNGA from HSA was detailed by Yang et al. (1). On average, 38 units of galactose were reported to be attached to each HSA molecule (1). The radiochemical yield of the final labeled product was typically 8–10%, and the time required to complete the entire procedure was 150 ± 20 min. The radiochemical purity of [^18^F]FNGA was >99% as determined with instant thin-layer chromatography (ITLC), with a specific activity of 1.92–7.10 TBq/mmol (51.8–191.7 Ci/mmol). [^18^F]FNGA was reported to be stable for >4 h in saline at room temperature and maintained a radiochemical purity of >95% as determined with ITLC. The purified radiocompound was also stable for >4 h when stored at 37°C in murine plasma as determined with high-performance liquid chromatography.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FNGA+in+vitro)]

No references are currently available.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20rodentia)]

Yang et al. investigated the biodistribution of [^18^F]FNGA in normal mice (1). The animals were injected with the radiochemical through the tail vein and euthanized at 5 min and 30 min (n = 5 mice per time point) after injection. Major tissues and organs were subsequently removed from the animals to determine the amount of accumulated radioactivity. The data was presented as percent of injected dose per gram tissue (% ID/g) for the various samples. To determine the binding specificity of [^18^F]FNGA, the animals (n = 5 mice) were injected with non-radioactive NGA (10 mg/kg body weight) followed by an injection of [^18^F]FNGA 5 min later. The animals were euthanized 5 min after treatment with the radiochemical, and samples were treated as before to determine the amount of radioactivity accumulated in the various tissues and organs.

Within 5 min of treatment with [^18^F]FNGA, >75% ID/g of the label was detected in the liver, and all the other organs (heart, lung, kidney, spleen, stomach, blood, muscle, and small intestine) showed an accumulation of <3% ID/g radioactivity at this time point (1). By 30 min after injection, radioactivity in the liver had reduced to <15% ID/g with an accumulation of ~17.5%ID/g in the kidneys. Compared with the normal animals, mice pretreated with a blocking dose of non-radioactive NGA had significantly (P < 0.01) less accumulation of radioactivity in the liver (<15% ID/g) at 5 min after injection of [^18^F]FNGA. In these animals, significantly (P < 0.01) increased radioactivity was detected in the blood (>45% ID/g), lungs (>15% ID/g), kidneys (>10% ID/g), and spleen (>5% ID/g), indicating that the radiolabeled compound bound specifically to the ASGP-R in the liver.

MicroPET imaging with [^18^F]FNGA was performed on rats (n = 1 mouse per group) with or without blocking with non-radioactive NGA as before (1). The images were acquired 5 min and 15 min after treatment with the radiotracer. From the images it was evident that the radiolabel accumulated in the liver within 5 min after injection, and by 15 min some of the radioactivity had been lost from this organ, although the liver outline was clearly visible. Low uptake of the radiotracer was observed in the kidneys, spleen, and other organs during this time. Treatment of the animals with non-radioactive NGA followed by an injection of [^18^F]FNGA was reported to reduce the level of accumulated radioactivity in the liver and make the outline of the organ unclear on imaging. During the same time period, the label was observed to accumulate in the kidney with quick clearance through the bladder.

From these studies the investigators concluded that [^18^F]FNGA can be used for imaging the liver in a preclinical setting and after further evaluation could help evaluate the risk of hepatic surgery in humans (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FNGA+Non-Primate+Mammals)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FNGA+Non-Human+Primates)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=18F+FNGA+Human+Studies)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## References

1 Yang W., Mou T., Peng C., Wu Z., Zhang X., Li F., Ma Y. (2009). Fluorine-18 labeled galactosyl-neoglycoalbumin for imaging the hepatic asialoglycoprotein receptor. Bioorg Med Chem.
2 Lee S.M., Casey C.A., McVicker B.L. (2009). Impact of asialoglycoprotein receptor deficiency on the development of liver injury. World J Gastroenterol.